# Gd-DOTA-anti-Aβ42-F(ab’)_2_-antibody fragment (putrescine)_n_

Chemical name: | Gd-DOTA-anti-Aβ42-F(ab’)_2_ -antibody fragment (putrescine)_n_
Abbreviated name: | GdAβ42
Synonym:
Agent category: | F(ab’)_2_ antibody fragment
Target: | Fibrillar Aβ42
Target category: | Antibody-antigen binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd + Ab42+ F(ab')2)]

Alzheimer disease (AD) is a neurodegenerative disease characterized by the accumulation of extracellular neuritic or senile plaques and neurofibrillary tangles (NFTs) in the human brain (1, 2). A neuritic plaque contains a dense core formed by amyloid-β peptides (Aβ), which are 39–43 amino acids in length and are derived from proteolytic cleavage of amyloid precursor protein (APP) by β- and γ-secretases. NFTs are formed by intraneuronal bundles of paired helical filaments mainly from the aggregates of hyperphosphorylated tau protein (2). Both types of deposits, each with a diameter of ~10 nm, are caused by aggregation of highly hydrophobic peptides and can generate significant neurotoxicity (3). The mechanism of Aβ plaque has been extensively studied in various animal models. For instance, four genes have been identified as related to the early onset of AD, including APP, human presenilin 1 (PS1), human presenilin 2 (PS2), and apolipoprotein E (ApoE) (2). Several transgenic models such as the APP single transgenic mouse (Tg2576), the PS1 single transgenic mouse (M146L6.2), or the APP/PS1 double transgenic mouse, produced by mating a Tg2576 mouse with a M146L6.2 mouse, have been developed to study AD (4). These animal models readily produce Aβ plaques in their brains and generate behavioral deficits (5, 6).

One of the promising therapeutic strategies for amyloid clearance is immunization against Aβ, either with active vaccination via Aβ injection or with intravenous administration of anti-Aβ antibodies (7). IgG4.1 is an anti-Aβ antibody that binds to the first 15 residues in soluble or fibrillar Aβ40/42, an Aβ that is 40 or 42 amino acids in length (4). A fragment with smaller molecular weight, F(ab’)_2_4.1, can be obtained by removal of the Fc portion in IgG4.1. Use of this fragment can minimize inflammatory response and reduce molecular weight for better diffusion through the blood brain barrier (BBB). In addition, polyamines such as putrescine (1,4-diaminobutane) can be conjugated to the fragment, which can increase the permeability at the BBB many fold (1). Gd-1,4,7,10-tetra-azacyclododecane-1,4,5,10-tetraacetic acid (DOTA)-anti-Aβ42-F(ab’)_2_-antibody fragment (putrescine)_n_ (GdAβ42) is a magnetic resonance imaging (MRI) agent used for imaging Aβ plaques in vivo (4). GdAβ42 consists of three components: Gd chelates (Gd-DOTA) for T_1_-relaxivity enhancement, an anti-Aβ42 antibody fragment F(ab’)_2_4.1 to bind Aβ plaques, and putrescine molecules that are covalently attached to the antibody fragment to enhance the BBB permeability.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd + Ab42+ F(ab')2)+AND+synthesis%0D%0A)]

Ramakrishnan et al. reported the preparation of GdAβ42 (4). Initially, antibody fragment F(ab’)_2_4.1 was obtained by digesting monoclonal antibody IgG4.1 using ficin at pH 6.5. Then the chelating agent DOTA was coupled to F(ab’)_2_4.1 via carbodiimide reaction in two steps: DOTA was activated with carbodiimide, followed by conjugation with the ε-amino group of lysine residues in the F(ab’)_2_4.1. The number of DOTA molecules was controlled to be 1–2 per F(ab’)_2_4.1. The obtained DOTA-F(ab’)_2_4.1 was reacted with GdCl_3_ to form Gd-DOTA-F(ab’)_2_4.1. The protein carboxylic acid groups of Gd-DOTA-F(ab’)_2_4.1 were further activated with 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide hydrochloride followed by conjugation with the primary amine group of putrescine to produce GdAβ42.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd + Ab42+ F(ab')2)+AND+%22in+vitro%22)]

Ramakrishnan et al. examined the binding of GdAβ42 to amyloid plaques in vitro (4). GdAβ42 was radiolabeled with ^125^I using the chloramine-T procedure. After incubation of ^125^I-labeled GdAβ42 with unfixed brain sections of an APP/PS1 double transgenic mouse for 3 h, the brain sections were dipped in an autoradiographic emulsion for ^125^I. The amyloid plaques in the mouse brain sections were found to be labeled with GdAβ42. Then the contrast enhancement of GdAβ42 in MRI was examined in vitro. GdAβ42 was incubated with unfixed brain slices (500 μm thick) from a 29-month-old APP transgenic mouse for 2 h, at which time T_1_-weighted images were collected with a 9.4-T imager with a voxel dimension of 60×60×120 μm^3^. In the slices containing hippocampus, the T_1_-weighted images exhibited many hyperintense foci (bright spots) throughout the cortex and hippocampus, which further confirmed the binding of GdAβ42 to the amyloid plaques. As a control, brain slices from a wild-type mouse were imaged, but they did not show any hyperintense foci in T_1_-weighted images.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd + Ab42+ F(ab')2) +AND++rodentia)]

Ramakrishnan et al. measured the plasma pharmacokinetics of GdAβ42 in mice (4). GdAβ42 was radiolabeled with ^125^I and injected intravenously into a 6-month-old wild-type mouse at a dose of 100 μCi (3.7 MBq). Series blood samples were collected over a period of time. ^125^I-GdAβ42 had a distribution rate constant of 0.037 ± 0.012 min^-1^ in the α-phase, an elimination rate constant of 0.005 ± 0.002 min^-1^ for the β-phase, a clearance of 0.0469 ± 0.0084 ml/min, and a maximum plasma concentration of 21.52 ± 0.76 μCi/ml (0.796 ± 0.028 MBq/ml). After the final blood sample, the mouse was euthanized and tissues were harvested for quantification of ^125^I radioactivity. The biodistribution of ^125^I-GdAβ42 was ~2% in brain and liver, <1% in heart and lung, ~3% in spleen, and ~ 4% in kidney. The permeability coefficient × surface area product (PS; ml·g^-1^s^-1^ × 10^-6^) was evaluated for six brain tissues: 39.8 ± 1.7 in cortex, 26.8 ± 1.2 in caudate-putamen, 48.0 ± 2.2 in hippocampus, 42.7 ± 1.9 in thalamus, 57.8 ± 2.6 in brainstem, and 56.0 ± 2.5 in cerebellum. Their corresponding vascular space (V_p_; μl/g) values were 24.8 ± 6.5 in cortex, 13.8 ± 4.3 in caudate-putamen, 32.7 ± 9.6 in hippocampus, 27.0 ± 7.9 in thalamus, 39.0 ± 9.4 in brainstem, and 38.9 ± 10.7 in cerebellum. Compared to the PS of 1–2 × 10^-6^ ml·g^-1^s^-1^ for native F(ab’)_2_4.1, the BBB permeability of ^125^I-GdAβ42 increased 18–33-fold, whereas their V_p_ appeared to be similar.

Ramakrishnan et al. also examined the in vivo labeling of amyloid plaques with ^125^I-GdAβ42 (4). APP/PS1 double transgenic mice (n = 5; 9 months old) were injected intravenously with ^125^I-GdAβ42 at a dose of 2 mCi (74 MBq). The animals were euthanized 4 h later and brain tissues were sectioned. The amyloid plaques were stained with anti-Aβ antibody, and the radiolabeled immunoglobins were detected with emulsion microautoradiography. The amyloid plaques were found to be labeled with ^125^I-GdAβ42 and distributed throughout the cortex and hippocampus, arising from an increased permeability of GdAβ42 at the BBB.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd + Ab42+ F(ab')2) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd + Ab42+ F(ab')2) +AND+human)]

No publication is currently available.

### NIH Support

NS 57091

## References

1 Wengenack T.M., Curran G.L., Poduslo J.F. (2000). Targeting alzheimer amyloid plaques in vivo. Nat Biotechnol.
2 Villemagne V.L., Fodero-Tavoletti M.T., Pike K.E., Cappai R., Masters C.L., Rowe C.C. (2008). The ART of loss: Abeta imaging in the evaluation of Alzheimer's disease and other dementias. Mol Neurobiol.
3 Goedert M., Spillantini M.G. (2006). A century of Alzheimer's disease. Science.
4 Ramakrishnan M., Wengenack T.M., Kandimalla K.K., Curran G.L., Gilles E.J., Ramirez-Alvarado M., Lin J., Garwood M., Jack C.R., Poduslo J.F. (2008). Selective contrast enhancement of individual Alzheimer's disease amyloid plaques using a polyamine and Gd-DOTA conjugated antibody fragment against fibrillar Abeta42 for magnetic resonance molecular imaging. Pharm Res.
5 Poduslo J.F., Ramakrishnan M., Holasek S.S., Ramirez-Alvarado M., Kandimalla K.K., Gilles E.J., Curran G.L., Wengenack T.M. (2007). In vivo targeting of antibody fragments to the nervous system for Alzheimer's disease immunotherapy and molecular imaging of amyloid plaques. J Neurochem.
6 Radde R. Duma C. Goedert M. Jucker M. The value of incomplete mouse models of Alzheimer's disease Eur J Nucl Med Mol Imaging 2008 35Suppl 1S70 4 18270700
7 Raymond S.B., Treat L.H., Dewey J.D., McDannold N.J., Hynynen K., Bacskai B.J. (2008). Ultrasound enhanced delivery of molecular imaging and therapeutic agents in Alzheimer's disease mouse models. PLoS ONE.